# N-4-[^18^F]Fluorobenzoyl-c(RGDyK)

Chemical name: | N-4-[^18^F]Fluorobenzoyl-c(RGDyK)
Abbreviated name: | [^18^F]FB-c(RGDyK), [^18^F]FB-RGD
Synonym:
Agent Category: | Peptide
Target: | Integrin α_v_β_3_
Target Category: | Receptor binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FB-RGD)]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell-cell and cell-matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. α_v_β_3_ antagonists are being studied as antitumor and antiangiogenic agents and the agonists as angiogenic agents for coronary angiogenesis (6, 8, 9). A tripeptide sequence consisting of Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various radiolabeled antagonists have been introduced for imaging of tumors and tumor angiogenesis (10).

Most of the cyclic RGD peptides are monomeric and composed of five amino acids. Haubner et al. (11) reported that various cyclic RGD peptides exhibit selective inhibition of binding to α_v_β_3_ (IC_50_, 7-40 nM) but not to α_v_β_5_ (IC_50_, 600-4,000 nM) or α_IIb_β_3_ (IC_50_, 700-5,000 nM) integrin. [^18^F]FB-c(RGDyK) was synthesized to study in vivo biodistribution of the tracer in tumor-bearing mice. [^18^F]FB-c(RGDyK) was found to have high accumulation in tumors, but it also had a high tumor washout and biliary excretion into the gallbladder and intestines (12). A dimeric analog was also synthesized as [^18^F]FB-E[c(RGDyK)]_2_, which was shown to have higher tumor uptake than the monomer and predominantly renal excretion (13).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FB-RGD%20and%20synthesis)]

N-Succinimidyl 4-[^18^F]fluorobenzoate ([^18^F]SFB) was synthesized in two steps from [^18^F]KF (Kryptofix 2.2.2./K_2_CO_3_) in 65 min (12). The decay-corrected yields of [^18^F]SFB were 60-65%, based on starting [^18^F]KF. [^18^F]SFB was used to conjugate c(RGDyK) and E[c(RGDyK)]_2_ to form [^18^F]FB-c(RGDyK) and [^18^F]FB-E[c(RGDyK)]_2_, respectively. Radiochemical purities >99% were obtained for both peptides, and radiochemical yields were 35-45% for the monomer and 20-30% for the dimers (12). The specific activity was 222 GBq/μmol (6 Ci/μmol) at end of synthesis. Total synthesis time was about 200 min including the final high-performance liquid chromatography purification.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FB-RGD%20and%20%28in%20vitro%20or%20cell%29)]

A receptor-binding assay (13) with ^125^I-c(RGDyK) was established using a primary human brain capillary endothelial cells, which contain α_v_β_3_ and α_v_β_5_ integrin. FB-c(RGDyK), FB-E[c(RGDyK)]_2_, c(RGDyK), and [c(RGDyK)]_2_ had IC_50_ values of 16.9 ± 0.5, 6.7 ± 0.5, 3.5 ± 0.3, and 2.3 ± 0.7 nM, respectively (13). Haubner et al. (11) showed that c(RGDyK(SAA)) had IC_50_ values of 20, 4,000, and 3,000 nM for α_v_β_3_, α_v_β_5_, and α_IIb_β_3_, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FB-RGD%20and%20rodentia)]

Chen et al. (12) performed biodistribution studies of [^18^F]FB-c(RGDyK) in nude mice, using a U87MG glioblastoma s.c. xenograft model. Data were obtained at 30, 60, and 120 min after injection. [^18^F]FB-c(RGDyK) had very rapid blood clearance, resulting in very low activity in the blood, bone, and muscle at 30, 60, and 120 min (<0.5% of injected dose (ID)/g). There was little defluorination of the tracer in the bone. The initial tracer accumulation in the α_v_β_3_-integrin-expressing U87MG tumor was about 3% ID/g at 30 min and decreased to about 1.5% ID/g at 2 h. Tumor uptake of radioactivity was blocked by co-injection of unlabeled c(RGDyK) from 2.6% ID/g to 0.35% ID/g (5 mg/kg) and 0.26% ID/g (15 mg/kg). The tracer had very fast renal clearance. At 60 min, the highest and second highest radioactive concentrations were found in the urine and gallbladder, followed by the tumor, kidney, and liver. Tumor/blood and tumor/muscle ratios at 2 h were high (21 and 8.2, respectively). [^18^F]FB-RGD demonstrated rapid blood clearance and fast tumor accumulation. [^18^F]FB-E[c(RGDyK)]_2_ showed a similar biodistribution profile in this tumor model except that tumor accumulation was significantly higher than for the monomer (13).

[^18^F]FB-c(RGDyK) positron emission tomography imaging studies in mice with an orthotopic U251T human brain tumor showed the tumor in the brain with low background in normal brain. c(RGDyK) pretreatment lowered the tumor/brain ratio from 8 to 2.5 (12).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FB-RGD%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FB-RGD%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FB-RGD%20and%20%28human%20not%20cell%29)]

No publication is currently available.

## NIH Support

P20 CA86532, R01 CA82989

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
11 Haubner R., Wester H.J., Burkhart F., Senekowitsch-Schmidtke R., Weber W., Goodman S.L., Kessler H., Schwaiger M. (2001). Glycosylated RGD-containing peptides: tracer for tumor targeting and angiogenesis imaging with improved biokinetics. J Nucl Med.
12 Chen X., Park R., Shahinian A.H., Tohme M., Khankaldyyan V., Bozorgzadeh M.H., Bading J.R., Moats R., Laug W.E., Conti P.S. (2004). 18F-labeled RGD peptide: initial evaluation for imaging brain tumor angiogenesis. Nucl Med Biol.
13 Chen X., Tohme M., Park R., Hou Y., Bading J.R., Conti P.S. (2004). Micro-PET imaging of alphavbeta3-integrin expression with 18F-labeled dimeric RGD peptide. Mol Imaging.